# 4-(2´-Methoxyphenyl)-1-[2´-(N-2´´-1,3 pyrimidino)-p-[^18^F]fluorobenzamido]ethylpiperazine

Chemical name: | 4-(2´-Methoxyphenyl)-1-[2´-(N-2´´-1,3 pyrimidino)-p-[^18^F]fluorobenzamido]ethylpiperazine
Abbreviated name: | [^18^F]FPWAY
Synonym: | [^18^F]FBWAY 1,3 N 4-[^18^F]-Fluoro-N-{2-[4-(2-methoxyphenyl)-1-piperazinyl]ethyl}-N-(2-pyrimidinyl)benzamide
Agent Category: | Compound
Target: | 5-HT_1A_ receptors
Target Category: | Receptor-ligand binding
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBWAY%201%2C3N%20OR%20FPWAY)]

4-(2´-Methoxyphenyl)-1-[2´-(N-2´´-1,3 pyrimidino)-p-[^18^F]fluorobenzamido]ethylpiperazine ([^18^F]FPWAY) is a radioligand developed for positron emission tomography (PET) imaging of serotonin-1A (5-HT_1A_) receptors in the central nervous system (1, 2). It is a selective 5-HT_1A_ antagonist labeled with ^18^F, a positron emitter with a physical t_½_ of 109.7 min (3, 4).

The serotonin (5-hydroxytryptamine (5-HT)) neurotransmission system consists mainly of neurons in the brainstem, with nerve tracts extending from these neurons to many areas of the brain and spinal cord. During firing, the neurons release 5-HT, a neurotransmitter that is involved in the modulation of various important physiologic functions and behavior, such as thermoregulation, cardiovascular function, aggressive and sexual behavior, mood, appetite, and the sleep–wake cycle. The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which also contain several subtypes. There are five receptor subtypes within the G protein-coupled 5-HT_1_ receptor family, with the 5-HT_1A_ subtype located primarily in the limbic forebrain (the hippocampus, entorhinal cortex and septum). 5-HT_1A_ receptors appear to function both as presynaptic (somatodendritic) autoreceptors in the raphe nuclei and as postsynaptic receptors in the terminal fields. This receptor subtype is involved in the modulation of emotion and the function of the hypothalamus, and is implicated in the pathogenesis of anxiety, depression, hallucinogenic behavior, motion sickness, dementia, schizophrenia, and eating disorders. A radioligand that can be used to assess the in vivo densities of 5-HT_1A_ receptors and their changes may facilitate investigation of the relationship of these receptors to various neuropsychiatric diseases and aid in the design of novel drugs for their treatment.

Many psychiatric drugs modulate serotonergic transmission or specifically target the 5-HT_1A_ receptors. Various compounds have been radiolabeled for visualization and quantification of these receptors. WAY 100635 was developed as a highly selective, silent antagonist (possessing no intrinsic agonist activity) of 5HT_1A_ receptors at both pre- and postsynaptic sites. WAY 100635 radiolabeled with ^11^C at the carbonyl position is an effective radioligand but it is rapidly cleared and metabolized. The short t_½_ of ^11^C also presents some challenges in clinical application of the radiotracer. A radioligand with slower metabolism and labeled with a longer-lived radioisotope would be a better agent for quantitative PET studies. A number of fluorinated derivatives of WAY 100635 have been developed. In 2000, Lang et al. (5) synthesized [^18^F]FPWAY with labeling at the carboxamide moiety to minimize metabolites that cross the blood-brain barrier (BBB). [^18^F]FPWAY appears to be an intermediate-affinity antagonist of the 5-HT_1A_ receptors and may be more sensitive to transient changes in endogenous 5-HT_1A_ levels than high-affinity analogs (6). In this WAY 100635 analog, the pyridine ring is replaced by pyrimidine and the cyclohexane ring is replaced by fluorobenzyl. With ^18^F in the 4 position of the benzamide, [^18^F]FPWAY is a very different compound from another WAY 100635 analog with a similar abbreviation, [^18^F]6FPWAY, which was synthesized by Marchais et al. (7). [^18^F]6FPWAY contains a N-pyridine with ^18^F in the 6 position of the pyridine moiety.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FBWAY%201%2C3N%20OR%20FPWAY%29%20AND%20synthesis)]

Lang et al. (5, 8) first reported the synthesis of FPWAY based on FBWAY (or p-MPPF). FPWAY was synthesized as an FBWAY analog (FBWAY 1,3 N) with a 1,3 pyrimidine substituent. FBWAY was prepared by reacting WAY 100634 with the corresponding acid chloride in methylene chloride. Radiolabeling involved labeling the 4-trimethylamino precursor with ^18^F to produce the radiolabeled 4-fluorobenzoyl chloride. The product was purified by high-performance liquid chromatography (HPLC). The radiochemical yield ranged between 10 and 20%, and the total synthesis time was between 80 and 90 min. The specific activity was 37,000 GBq (1,000 Ci)/mmol at the end of bombardment (EOB).

Ma et al. (9) described a similar synthesis of FPWAY from {2-[4-(2-methoxyphenyl)-1-piperazinyl]-ethyl}-N-(2-pyrimidinyl)amine which was prepared from 2-[4-(2-methoxyphenyl)-1-piperazinyl]ethylamine (obtained commercially) by reaction with 2-chloropyrimidine in ethanol and sodium carbonate overnight. The yield was 79%. The final compound was reacted with 4-fluorobenzoyl chloride in triethylamine and 1,2-dichloroethane overnight to give a final yield of 96%. This precursor was reacted with [^18^F]− Kryptofix in dimethyl sulfoxide and heated in a microwave oven for 2 min. The product was purified by reverse-phase HPLC and a C-18 Sep-Pak to give a final yield of 25-35% EOB and radiochemical purity of 99.0%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FBWAY%201%2C3N%20OR%20FPWAY%29%20AND%20in%20vitro%20studies)]

In vitro affinity of [^18^F]FPWAY was studied by Lang et al. (5), and the inhibition constant, K_i_, was determined to be <1 nM against [^18^H]8-hydroxy-2-dipropylaminotetralin ([^3^H]8-OH-DPAT) binding to a cloned cell line containing 5-HT_1A_ receptors. This was relatively weak when compared with other high affinity WAY analogs (MeFWAY and Trans-FCWAY). The antagonist inhibition concentration (IC_50_)was determined to be 340 nM based on the compound’s ability to inhibit relaxation induced by 0.3 µM 8-OH-DPAT. On the basis of the compound’s ability to relax guinea pig field-stimulated ileum, the authors concluded that [^18^F]FPWAY showed no agonist activity.

In vitro metabolism studies of FPWAY and [^18^F]FPWAY were performed by Ma et al. (9) in cryopreserved hepatocytes of rat and human liver tissue. Metabolites were identified by liquid chromatography−tandem mass spectrometry. In rat hepatocytes, aromatic-ring oxidation was the major metabolism pathway for FPWAY, but there was also amide hydrolysis. Amide hydrolysis products were the major metabolites of FPWAY in human hepatocytes, and the metabolic rate appeared to be higher than for other fluorinated analogs of WAY 100635 (FBWAY and MeFBWAY). The study suggested that the pyrimidyl for pyridyl substitution in FPWAY made the amide more labile to metabolic hydrolysis. In a [^18^F]FPWAY imaging study using monkey blood, it was shown that pure [^18^F]FPWAY could be readily extracted by an organic phase (hexane−etyhl acetate 4:1) from its metabolites in a basic aqueous phase (125 mM KCl-NaOH, pH 12.5). This simplified the determination of the input function.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FBWAY%201%2C3N%20OR%20FPWAY%29%20AND%20rodentia)]

Lang et al. (5) studied the clearance of [^18^F]FPWAY from the rat brain by injecting the compound into rats. [^18^F]FPWAY appeared to have a two-component net efflux curve. Brain distribution and binding saturability were also determined in rats. The differential uptake ratios (DURs, calculated as % of injected dose x animal weight (g)/100) of [^18^F]FPWAY at 30 min were 0.403 ± 0.056 (n ≥ 4), 0.918 ± 0.107, and 0.141 ± 0.019 for the cortex, hippocampus, and cerebellum, respectively. When 200 nmol of WAY 100635 was co-injected along with [^18^F]FPWAY, the DURs decreased to 0.153 ± 0.040, 0.145 ± 0.040, and 0.131 ± 0.033 for the cortex, hippocampus, and cerebellum, respectively. The hippocampus/cerebellum ratios were 5.5 and 0.1 with and without 200 nM WAY 100635, respectively. The kinetic sensitivity (change in DUR per change in receptor concentration) of this compound appeared to be intermediate between FCWAY and FBWAY.

Jagoda et al. (10) conducted autoradiography, biodistribution, and metabolite studies of [^18^F]FPWAY and other analogs ([^18^F]FCWAY and [^18^F]FBWAY) in rats and mice. The DURs (dose = 1850 kBq (50 µCi); n = 5) in rats at 30 min after injection for the hippocampus and cerebellum were 0.92 ± 0.11 and 0.14 ± 0.02, respectively. Their (hippocampus DUR/cerebellum DUR) − 1 ratio ((H/Cb) − 1) was 5.5. With the administration of WAY 100635 (200 nmol), the DURs for the hippocampus and cerebellum decreased to 0.14 ± 0.04 and 0.13 ± 0.03, respectively. The specific binding ratios (hippocampus/cerebellum) were 9, 4.6, and 0.1 for the mice of wildtype, heterozygotes, and receptor knockout mice, respectively. This showed that [^18^F]FPWAY bound specifically to the 5-HT_1A_ receptors and was sensitive to changes in receptor density. Similar differences in localization patterns were observed in [^18^F]FPWAY autoradiography studies. The results from the blocking studies with WAY 100635 in rat and mouse brains were consistent with the fact that [^18^F]FPWAY possesses a lower 5HT_1A_ receptor affinity than do high-affinity analogs. [^18^F]FPWAY regional bindings in the brains of “awake” mice showed no significant changes in response to treatments with paroxetine (a selective serotonin reuptake inhibitor) or fenfluramine (a serotonin transporter substrate and releasing agent). With use of the “chase” paradigm, a consistent pattern of changes of [^18^F]FPWAY regional brain binding in awake rats treated with fenfluramine or paroxetine was not observed. Urethane-anesthetized rats treated with fenfluramine also showed no significant changes in the specific binding ratios in the hippocampus. The study suggested that the in vivo serotonin system is tightly controlled so that changes in radioligand affinity alone might not produce significant changes in detection sensitivity for changes in endogenous 5-HT.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FBWAY%201%2C3N%20OR%20FPWAY%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FBWAY%201%2C3N%20OR%20FPWAY%29%20AND%20%28primate%20NOT%20human%29)]

Carson et al. (11) studied the brain penetration of [^18^F]fluorobenzoic acid ([^18^F]FB), a major acid metabolite of [^18^F]FPWAY, in rhesus monkeys. PET imaging showed that [^18^F]FB crossed the BBB, but it did not have a significant effect on 5-HT_1A_ receptor quantification of [^18^F]FPWAY. HPLC analysis of arterial blood samples also showed no metabolites when [^18^F]FB was injected.

Giovacchini et al. (6) used PET imaging (10-40 min after injection) in rhesus monkeys to assess the response of [^18^F]FPWAY to dynamic in vivo changes in serotonergic neurotransmission caused by systemic administration of paroxetine. A dose of 259-518 MBq (7-14 mCi) of [^18^F]FPWAY (specific activity was 111 GBq (3 Ci/µmol) at time of administration), TOA) was given with a bolus-plus-infusion technique to achieve constant radioactivity in all brain regions. The distribution of radioactivity in the brain was consistent with the known concentrations of 5-HT_1A_ receptors. The baseline binding potential (BP_2_) values of the raphe region, anterior cingulated, and frontal lobe were 0.53 ± 0.06, 1.90 ± 0.08, and 0.93 ± 0.08, respectively. Paroxetine administration (5 mg/kg) caused decreases of raphe BP_2_s ranging from 8 ± 6% during the first 30 min period to 27 ± 10% during the sixth 30-min period (180-240 min). On the other hand, cortical BP_2_ values increased by 7 ± 3% during the first 30-min period and by 13 ± 5% during the second 30-min period, and then progressively decreased. The study suggested that dynamic changes in 5-HT_1A_ neurotransmission could be quantified by [^18^F]FPWAY PET imaging.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FBWAY%201%2C3N%20OR%20FPWAY%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH Intramural Support. NIH Contract NO1MH2003.

## References

1 Passchier J., van Waarde A. (2001). Visualisation of serotonin-1A (5-HT1A) receptors in the central nervous system. Eur J Nucl Med.
2 McCarron J.A., Pike V.W., Halldin C., Sandell J., Sovago J., Gulyas B., Cselenyi Z., Wikstrom H.V., Marchais-Oberwinkler S., Nowicki B., Dolle F., Farde L. (2004). The pyridinyl-6 position of WAY-100635 as a site for radiofluorination--effect on 5-HT1A receptor radioligand behavior in vivo. Mol Imaging Biol.
3 Bantick R.A., Rabiner E.A., Hirani E., de Vries M.H., Hume S.P., Grasby P.M. (2004). Occupancy of agonist drugs at the 5-HT1A receptor. Neuropsychopharmacology.
4 Karramkam M., Hinnen F., Berrehouma M., Hlavacek C., Vaufrey F., Halldin C., McCarron J.A., Pike V.W., Dolle F. (2003). Synthesis of a [6-pyridinyl-18F]-labelled fluoro derivative of WAY-100635 as a candidate radioligand for brain 5-HT1A receptor imaging with PET. Bioorg Med Chem.
5 Lang L., Jagoda E., Schmall B., Sassaman M., Ma Y., Eckelman W.C. (2000). Fluoro analogs of WAY-100635 with varying pharmacokinetics properties. Nucl Med Biol.
6 Giovacchini G., Lang L., Ma Y., Herscovitch P., Eckelman W.C., Carson R.E. (2005). Differential effects of paroxetine on raphe and cortical 5-HT1A binding: a PET study in monkeys. Neuroimage.
7 Marchais S., Nowicki B., Wikstrom H., Brennum L.T., Halldin C., Pike V.W. (2001). Short and efficient syntheses of analogues of WAY-100635: new and potent 5-HT1A receptor antagonists. Bioorg Med Chem.
8 Lang L., Jagoda E., Schmall B., Vuong B.K., Adams H.R., Nelson D.L., Carson R.E., Eckelman W.C. (1999). Development of fluorine-18-labeled 5-HT1A antagonists. J Med Chem.
9 Ma Y., Lang L., Kiesewetter D.O., Eckelman W.C. (2002). Liquid chromatography-tandem mass spectrometry identification of metabolites of three phenylcarboxyl derivatives of the 5-HT(1A) antagonist, N-(2-(4-(2-methoxyphenyl)-1-piperazinyl)ethyl)-N-(2-pyridyl) trans-4-fluorocyclohexanecarboxamide (FCWAY), produced by human and rat hepatocytes. J Chromatogr B Analyt Technol Biomed Life Sci.
10 Jagoda E.M., Lang L., Tokugawa J., Simmons A., Ma Y., Contoreggi C., Kiesewetter D., Eckelman W.C. (2006). Development of 5-HT(1A) receptor radioligands to determine receptor density and changes in endogenous 5-HT. Synapse.
11 Carson R.E., Wu Y., Lang L., Ma Y., Der M.G., Herscovitch P., Eckelman W.C. (2003). Brain uptake of the acid metabolites of F-18-labeled WAY 100635 analogs. J Cereb Blood Flow Metab.